# ^68^Ga-Labeled DOTA-conjugated sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], a sulfated cholecystokinin 8 (sCCK8) peptide derivative

Chemical name: | ^68^Ga-Labeled DOTA-conjugated sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], a sulfated cholecystokinin 8 (sCCK8) peptide derivative
Abbreviated name: | [^68^Ga]sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^
Synonym:
Agent Category: | Peptide
Target: | Cholecystokinin receptor 2 (CCK2R)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cck2%20receptor&cmd=DetailsSearch)]

The three subtypes of the cholecystokinin (CCK) receptor (CCKR), designated CCK1R, CCK2R, and CCK2i4svR, belong to the G-protein–coupled receptor family and are classified on the basis of their affinities for the CCK and the gastrin peptides, differential distribution in the tissues, and molecular structure (1). The CCK1R (previously known as CCKA) is found mainly on the peripheral cells of the pancreas and has a 500- to 1,000-fold higher affinity for sulfated CCK8 (sCCK8; contains a sulfated tyrosine (Tyr) residue) compared with the non-sulfated ligand. In addition, CCK1R is expressed mainly in organs of the gastrointestinal tract of rodents, but it is expressed at low levels in humans (2). CCK2R (previously known as CCKB, also designated as the gastrin receptor (GR)) is expressed in the brain, stomach, pancreas, and gallbladder and exhibits an almost equivalent affinity for gastrin and sulfated or non-sulfated CCK. Although CCK1R and CCK2R/GR are expressed in several normal tissues, CCK2R is overexpressed in most cancerous tumors, such as medullary thyroid carcinomas (http://www.cancer.gov/cancertopics/pdq/genetics/medullarythyroid/HealthProfessional) (>90%), astrocytomas (http://www.cancer.gov/dictionary?cdrid=45602) (>65%), and stromal ovarian cancers (http://www.cancer.gov/cancertopics/types/ovarian) (100%). The CCK2i4svR is a splice variant of the CCK2R that is expressed only in colorectal and pancreatic neoplasms and is not detectable in normal colorectal mucosa (1). Several gastrin and CCK8 analogs that have a high affinity for CCK2R have been developed and labeled with radionuclides for the detection and therapy of these cancers. It has been shown that radiolabeled CCK8 derivatives and minigastrin (MG0; a shorter version of human gastrin 1 that consists of amino acids 5–17 of the parent peptide) can be used with scintigraphy to detect colorectal or pancreatic cancer tumors that overexpress CCK2i4svR (3) or to screen for patients who may benefit from the radiotherapy of this disease (4). In preclinical studies, however, a high uptake of radioactivity in the kidneys was observed with these radiochemicals, and it was concluded that these tracers will be of limited use in humans (5). In addition, the sulfated Tyr residue at position 2 in sCCK8 is rapidly hydrolyzed, and the two methionine (Met) residues at positions 3 and 6 in the peptide can be easily oxidized during radiolabeling procedures or under in vivo conditions (6).

Two cyclized MG analogs, cyclo-MG1 and cyclo-MG2, were synthesized, labeled with ^99m^Tc, and evaluated with single-photon emission computed tomography (SPECT) for the detection of tumors that express CCKR (7). Although the two ^99m^Tc-labeled cyclo-compounds were suitable for the detection of tumors, they had low in vitro stability and generated low-quality scintigraphic images because they rapidly degraded under in vivo conditions. Similar observations have been reported with other ^99m^Tc-labeled compounds that were used in clinical trials for the visualization of tumors that overexpressed the CCK2R (8). In an ongoing effort to develop imaging agents that can be used to visualize tumors that express CCK2R, a stabilized sCCK8 derivative was prepared by replacing the sulfated Tyr in the molecule with a sulfated phenylalanine (Phe^2^(p-CH_2_SO_3_H)) and by substituting the Met residues in the peptide with either norleucine (Nle) (sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^]) or homoproparglyglycine (HPG; sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^]) (6). To facilitate the radiolabeling of these compounds with radionuclides such as ^111^In or ^68^Ga, the different peptides, including sCCK8, were conjugated with 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA). In one study the sCCK8, sCCK8[Phe^2^(p-CH_2_SO_3_H), sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] and sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] peptides were labeled with ^111^In, and their biodistribution was compared in athymic BALB/c nude mice bearing AR42J (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1492&Template=cellBiology) cell tumors that express CCK2R (6). In another study, the biodistribution and noninvasive imaging characteristics of [^111^In/^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] were compared with those of [^111^In/^68^Ga]-DOTA-sCCK8 and [^111^In/^68^Ga]-DOTA-MG0 in athymic BALB/c nude mice bearing tumors generated from A431 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology) cells transfected with CCK2R (A431-CCK2R cells) (9). This chapter describes studies performed only with the ^68^Ga-labeled peptides. Results obtained with the ^111^In-labeled peptides are described in a separate chapter of MICAD (www.micad.nih.gov) (10).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=CCKR+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Mouse cholecystokinin B receptor (CCK2R (http://www.ncbi.nlm.nih.gov/gene/12426)); NCBI-Gene ID: 12426

Mouse CCK2R nucleotide and protein (http://www.genome.jp/dbget-bin/www_bget?mmu:12426) sequences in Kyoto Encyclopedia of Genes and Genomes database (KEGG)

KEGG pathway (Mouse CCK2R (http://www.genome.jp/dbget-bin/get_linkdb?-t+pathway+mmu:12426))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=cholecystokinin+receptor) related to cholecystokinin receptor

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20synthesis&cmd=DetailsSearch)]

The synthesis of [^68^Ga]-DOTA-sCCK8, [^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^68^Ga]-DOTA-MG0 has been described elsewhere (9). The radiochemical yield, radiochemical purity, and specific activity of the ^68^Ga-labeled peptides were not reported (9).

The ^68^Ga-labeled peptides used for positron emission tomography (PET) imaging were reported to have a specific activity of 50–58 MBq/nmol (1.85–2.15 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20in%20vitro%20studies&cmd=DetailsSearch)]

A competitive binding assay with A431-CCK2R cells was used to determine the apparent IC_50_ values of nonradioactive ^69^Ga-conjugated DOTA-sCCK8, DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and DOTA-MG0 (9). The IC_50_ values for the peptides were reported to be 0.83 ± 0.08 nM, 16.54 ± 0.06 nM, and 5.91 ± 0.06 nM, respectively. This indicated that, among the different CCK2R ligands used in this study, the [^69^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] peptide had the lowest affinity for the receptor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^68^Ga]-DOTA-sCCK8, [^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^68^Ga]-DOTA-MG0 was investigated in athymic BALB/c nude mice bearing A431-CCK2R cell tumors (9). The animals (n = 5 mice/group for each labeled peptide) were injected intravenously with 2 MBq (74 μCi; 0.03 nmol) of the peptide, and the rodents were euthanized at 1 h postinjection (p.i.) to determine the amount of radioactivity that accumulated in the various tissues, including the tumors. For blocking studies, the animals (n = 3 mice/labeled peptide) were injected with the tracer in the presence of 1,000-fold molar excess nonradioactive DOTA-sCCK8. Results obtained from this study were presented as percentage of injected dose per gram tissue (% ID/g).

With [^68^Ga]-DOTA-sCCK8 and [^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], the uptake of radioactivity in the tumors was 7.48 ± 0.42% ID/g and 6.35 ± 1.41% ID/g, respectively, compared with 14.2 ± 4.06% ID/g for [^68^Ga]-DOTA-MG0. The uptake of label in the pancreas was highest with [^68^Ga]-DOTA-sCCK8 (~13.0% ID/g), followed by [^68^Ga]-DOTA-MG0 (~6.0% ID/g) and [^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] (~2.5% ID/g) (9). A very high accumulation of tracer was observed in the kidneys (>75% ID/g) with [^68^Ga]-DOTA-MG0, compared with <1.0% ID/g for the other two labeled peptides. All other organs (blood, lungs, muscle, spleen, and small intestines) showed label accumulation of <0.5% ID/g with each of the ^68^Ga-labeled peptides. Accumulation of tracer in the different tissues was blocked by at least 50% when an excess concentration of nonradioactive sCCK8 was co-injected with the radiolabeled peptides. This indicated that the uptake of label in the tumors and the other tissues was mediated specifically through CCK2R.

MicroPET/computed tomography images of mice injected with the different ^68^Ga-labeled peptides were acquired for 30 min as described by Joosten et al. (9). The tumors were clearly visible at 1 h p.i. with each of the labeled peptides. In addition to the tumors, the intestines of the animals were visible with both [^68^Ga]-DOTA-sCCK8 and [^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^]. Radioactivity was also detected in the bladder with [^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^]. With [^68^Ga]-DOTA-MG0, a very high uptake of label was observed in the kidneys, but very little radioactivity was detected in these organs with the other two labeled peptides.

From these studies, the investigators concluded that the ^68^Ga-labeled analogs of sCCK8 are probably suitable for the noninvasive visualization and characterization of CCK2R in rodents. However, more work is necessary to exploit the full potential of these probes for the PET imaging of CCKR (9).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111in-labeled%20cck8%20peptide%20on%20human%20primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111in-labeled%20cck8%20peptide%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Laverman P., Sosabowski J.K., Boerman O.C., Oyen W.J. (2012). Radiolabelled peptides for oncological diagnosis. Eur J Nucl Med Mol Imaging.
2 Roosenburg S., Laverman P., van Delft F.L., Boerman O.C. (2011). Radiolabeled CCK/gastrin peptides for imaging and therapy of CCK2 receptor-expressing tumors. Amino Acids.
3 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.
4 von Guggenberg E., Dietrich H., Skvortsova I., Gabriel M., Virgolini I.J., Decristoforo C. (2007). 99mTc-labelled HYNIC-minigastrin with reduced kidney uptake for targeting of CCK-2 receptor-positive tumours. Eur J Nucl Med Mol Imaging.
5 von Guggenberg E., Rangger C., Sosabowski J., Laverman P., Reubi J.C., Virgolini I.J., Decristoforo C. (2012). Preclinical Evaluation of Radiolabeled DOTA-Derivatized Cyclic Minigastrin Analogs for Targeting Cholecystokinin Receptor Expressing Malignancies. Mol Imaging Biol.
6 Roosenburg S., Laverman P., Joosten L., Eek A., Oyen W.J., de Jong M., Rutjes F.P., van Delft F.L., Boerman O.C. (2010). Stabilized (111)In-labeled sCCK8 analogues for targeting CCK2-receptor positive tumors: synthesis and evaluation. Bioconjug Chem.
7 von Guggenberg E., Sallegger W., Helbok A., Ocak M., King R., Mather S.J., Decristoforo C. (2009). Cyclic minigastrin analogues for gastrin receptor scintigraphy with technetium-99m: preclinical evaluation. J Med Chem.
8 Kosowicz J., Mikolajczak R., Czepczynski R., Ziemnicka K., Gryczynska M., Sowinski J. (2007). Two peptide receptor ligands (99m)Tc-EDDA/HYNIC-Tyr(3)-octreotide and (99m)Tc-EDDA/HYNIC-(D)Glu-octagastrin for scintigraphy of medullary thyroid carcinoma. Cancer Biother Radiopharm.
9 Joosten L., Laverman P., Boerman O.C., Roosenburg S., Eek A., Rutjes F.P., van Delft F.L. (2012). In vitro and in vivo characterization of three 68Ga- and 111 In-labeled peptides for cholecystokinin receptor imaging. Mol Imaging.
10 Chopra, A., 111In-Labeled DOTA conjugate of sCCK8[Phe2(p-CH2SO3H),Nle3,6], a sulfated cholecystokinin 8 (sCCK8) peptide derivative Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 to current.